# ^86^Y-CHX-A''-diethylenetriamine pentaacetic acid-panitumumab

Chemical name: | ^86^Y-CHX-A''-diethylenetriamine pentaacetic acid-panitumumab
Abbreviated name: | ^86^Y-CHX-A''-DTPA-Panitumumab
Synonym:
Agent category: | Chimeric monoclonal antibody
Target: | Epidermal growth factor receptor (EGFR, HER1)
Target category: | Receptor
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^86^Y
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&val=4503491), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?val=NM_001963.2) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=Graphics&list_uids=1950) for more information about EGF.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=86Y%20panitumumab)]

Epidermal growth factor (EGF) is a 53-amino-acid cytokine (6.2 kDa) secreted by ectodermic cells, monocytes, kidneys, and duodenal glands (1). EGF stimulates growth of epidermal and epithelial cells. EGF and at least seven other growth factors and their transmembrane receptor kinases play important roles in cell proliferation, survival, adhesion, migration, and differentiation. The EGF receptor (EGFR) family consists of four transmembrane receptors, including EGFR (HER1/erbB-1), HER2 (erbB-2/neu), HER3 (erbB-3), and HER4 (erbB-4) (2). HER1, HER3, and HER4 comprise three major functional domains: an extracellular ligand-binding domain, a hydrophobic transmembrane domain, and a cytoplasmic tyrosine kinase domain. No ligand has been clearly identified for HER2. However, HER2 can be activated as a result of ligand binding to other HER receptors with the formation of receptor homodimers and/or heterodimers (3). HER1 as well as HER2 are overexpressed on many solid tumor cells, such as breast, non–small-cell lung, head and neck, and colon cancers (4-6). The high levels of HER1 and HER2 expression on cancer cells are associated with a poor prognosis (7-10).

Trastuzumab (a humanized immunoglobulin G_1_ (IgG_1_) monoclonal antibody (mAb) against the extracellular domain of recombinant HER2) (11) has been labeled as ^111^In-trastuzumab (12-14). C225 mAb (an anti-EGFR, mouse-human chimeric, monoclonal IgG_1_ antibody, also known as cetuximab) has been labeled as ^99m^Tc-EC-C225 for use with single-photon emission computed tomography (SPECT) imaging of EGFR expression on solid tumors (15, 16). However, positron emission tomography (PET) offers better sensitivity, resolution, and quantification than SPECT (17). ^64^Cu is an attractive radionuclide for labeling cetuximab. Panitumumab has been approved by the United States Food and Drug Administration as a single agent for the treatment of EGFR-expressing, metastatic, colorectal carcinoma. For evaluation as a PET imaging agent, ^64^Cu (t_1/2_ = 12.7 h) was attached to panitumumab via 1,4,7,10-tetraazacyclododecane-N,N',N'',N'''-tetraacetic acid (DOTA) to form ^64^Cu-DOTA-panitumumab. Niu et al. (18) performed ^64^Cu-DOTA-panitumumab PET imaging studies in nude mice bearing human head and neck squamous cell carcinoma tumors with different expressions of EGFR. Nayak et al. (19) prepared ^86^Y-CHX-A''-diethylenetriamine pentaacetic acid (DTPA)-panitumumab (^86^Y, t_1/2_ = 14.7 h) for quantitative PET of HER1-expressing carcinoma. ^86^Y was chosen because of its suitability for internalizing mAbs, well-established chemistry, and potential use of ^90^Y for radiotherapy.

### Related Resource Links:

- Chapters in MICAD (EGFR (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=EGFR+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad))
- Gene information in NCBI (EGFR (http://www.ncbi.nlm.nih.gov/gene/1956))
- Articles in OMIM (EGFR (http://www.ncbi.nlm.nih.gov/omim/131550))
- Clinical trials (Trastuzumab (http://www.clinicaltrials.gov/ct2/results?term=Trastuzumab), cetuximab (http://www.clinicaltrials.gov/ct2/results?term=Cetuximab), panitumumab (http://www.clinicaltrials.gov/ct2/results?term=panitumumab))
- Drug information in FDA (Trastuzumab (http://google2.fda.gov/search?q=Trastuzumab&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=11&y=14), cetuximab (http://google2.fda.gov/search?q=Cetuximab&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=7&y=18), panitumumab (http://google2.fda.gov/search?q=panitumumab&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=15&y=14))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=86Y%20panitumumab%20and%20synthesis)]

Bifunctional CHX-A''-DTPA was used to conjugate panitumumab to form CHX-A''-DTPA-panitumumab (~150 kD), which was purified with column chromatography (19). There were 1.6 DTPA molecules per antibody. Next, ^86^Y solution (140–170 MBq (3.8–4.6 mCi)) was added to CHX-A''-DTPA-panitumumab (0.33 nmol) in ammonium acetate buffer (pH 5–6). The reaction mixture was incubated for 30 min at room temperature, and ^86^Y-CHX-A''-DTPA-panitumumab was purified with column chromatography. The yield of ^86^Y-CHX-A''-DTPA-panitumumab was 60%–75% with a specific activity of ~375 MBq/nmol (10 mCi/nmol). Radiochemical purity was not given, but ^86^Y-CHX-A''-DTPA-panitumumab exhibited excellent stability after storage in the refrigerator for 1 d at 4°C.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=86Y%20panitumumab%20and%20in%20vitro)]

Nayak et al. (19) performed ^86^Y-CHX-A″-DTPA-panitumumab binding to fixed A431 cells, demonstrating good in vitro immunoreactivity (73.5 ± 4.8%) and low nonspecific binding (3.8 ± 1.7%) (n = 4).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=86Y%20panitumumab%20and%20rodentia)]

Nayak et al. (19) performed ex vivo biodistribution studies in nude mice (n = 4/group) bearing HER1-expressing human colorectal LS-174T (low EGFR expression) and prostate PC-3 (moderate EGFR expression) xenografts at 1-4 d after injection of 0.5 MBq (0.14 mCi, 0.03 nmol) ^86^Y-CHX-A''-DTPA-panitumumab. Accumulation into LS-174T tumors was high, with 28.4 ± 3.0% injected dose/gram (ID/g) and 34.3 ± 3.5% ID/g at 1 d and 4 d after injection, respectively. The tumor/blood ratios were 2.0 and 4.7 at 1 d and 4 d after injection, respectively. Accumulation into PC-3 tumors was 14.5 ± 1.3% ID/g and 27.6 ± 2.8% ID/g at 1 and 4 d after injection, respectively, with tumor/blood ratios of 1.3 and 3.2 at 1 d and 4 d after injection, respectively. On the other hand, normal tissues exhibited lower radioactivity than the tumors, with little change from 1 d to 4 d after injection. Co-injection of panitumumab (0.7 nmol) with ^86^Y-CHX-A''-DTPA-panitumumab was performed in mice bearing LS-174T, PC-3, and human epidermoid A431 (high EGFR expression) tumor xenografts. Radioactivity in the tumors and non-tumor tissues was measured at 3 d after injection. The accumulation in the non-blocked tumors was 34.7 ± 5.9% ID/g, 22.1 ± 1.9% ID/g, and 22.7 ± 1.7% ID/g, respectively. The accumulation in the blocked tumors was 9.3 ± 1.5% ID/g, 8.8 ± 0.9% ID/g, and 10.0 ± 1.3% ID/g, respectively. By contrast, little inhibition was observed in the non-tumor tissues. The mean tumor residence times were similar in the three tumors (2.7–2.8 d). The low HER1-expressing LS-174T tumors showed the highest accumulation of ^86^Y-CHX-A''-DTPA-panitumumab. This apparent dichotomy (LS-174T versus PC-3 and A431) may be explained by the fact that in vivo tumor accumulation is dependent on many physiological factors, such as tumor vasculature, blood flow, tumor interstitial pressure, factors present in the tumor microenvironment, and antigen shedding. Niu et al. (18) also reported the discrepancies of ^64^Cu-DOTA-panitumumab in tumor uptake and ex vivo HER1 expression levels determined with immunohistochemistry.

Nayak et al. (19) studied the whole-body distribution of ~2 MBq (0.054 mCi) ^86^Y-CHX-A''-DTPA-panitumumab with microPET imaging in the three xenograft tumor models in mice (n = 3/group) with static scans at various time points (0.5–3 d). The accumulation of ^86^Y-CHX-A''-DTPA-panitumumab was clearly visible in all the tumors at 1–3 d after injection. Co-injection of panitumumab inhibited accumulation of radioactivity in the tumors. There was a good correlation (r^2^ = 0.87) between the tracer accumulation in the tumors measured with microPET and that measured with ex vivo biodistribution studies.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=86Y%20panitumumab%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=86Y%20panitumumab%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=86Y%20panitumumab%20and%20human)]

No publication is currently available.

## NIH Support

Intramural Research Program

## References

1 Carpenter G., Cohen S. (1990). Epidermal growth factor. J Biol Chem.
2 Yarden Y. (2001). The EGFR family and its ligands in human cancer: signalling mechanisms and therapeutic opportunities. Eur J Cancer.
3 Rubin I., Yarden Y. (2001). The basic biology of HER2. Ann Oncol.
4 Grunwald V., Hidalgo M. (2003). Developing inhibitors of the epidermal growth factor receptor for cancer treatment. J Natl Cancer Inst.
5 Mendelsohn J. (1990). Anti-epidermal growth factor receptor monoclonal antibodies as potential anti-cancer agents. J Steroid Biochem Mol Biol.
6 Yasui W., Sumiyoshi H., Hata J., Kameda T., Ochiai A., Ito H., Tahara E. (1988). Expression of epidermal growth factor receptor in human gastric and colonic carcinomas. Cancer Res.
7 Ang K.K., Berkey B.A., Tu X., Zhang H.Z., Katz R., Hammond E.H., Fu K.K., Milas L. (2002). Impact of epidermal growth factor receptor expression on survival and pattern of relapse in patients with advanced head and neck carcinoma. Cancer Res.
8 Costa S., Stamm H., Almendral A., Ludwig H., Wyss R., Fabbro D., Ernst A., Takahashi A., Eppenberger U. (1988). Predictive value of EGF receptor in breast cancer. Lancet.
9 Ethier S.P. (1995). Growth factor synthesis and human breast cancer progression. J Natl Cancer Inst.
10 Yarden Y. (2001). Biology of HER2 and its importance in breast cancer. Oncology.
11 Carter P., Presta L., Gorman C.M., Ridgway J.B., Henner D., Wong W.L., Rowland A.M., Kotts C., Carver M.E., Shepard H.M. (1992). Humanization of an anti-p185HER2 antibody for human cancer therapy. Proc Natl Acad Sci U S A.
12 Perik P.J., Lub-De Hooge M.N., Gietema J.A., van der Graaf W.T., de Korte M.A., Jonkman S., Kosterink J.G., van Veldhuisen D.J., Sleijfer D.T., Jager P.L., de Vries E.G. (2006). Indium-111-labeled trastuzumab scintigraphy in patients with human epidermal growth factor receptor 2-positive metastatic breast cancer. J Clin Oncol.
13 Lub-de Hooge M.N., Kosterink J.G., Perik P.J., Nijnuis H., Tran L., Bart J., Suurmeijer A.J., de Jong S., Jager P.L., de Vries E.G. (2004). Preclinical characterisation of 111In-DTPA-trastuzumab. Br J Pharmacol.
14 Garmestani K., Milenic D.E., Plascjak P.S., Brechbiel M.W. (2002). A new and convenient method for purification of 86Y using a Sr(II) selective resin and comparison of biodistribution of 86Y and 111In labeled Herceptin. Nucl Med Biol.
15 Schechter N.R., Wendt R.E., Yang D.J., Azhdarinia A., Erwin W.D., Stachowiak A.M., Broemeling L.D., Kim E.E., Cox J.D., Podoloff D.A., Ang K.K. (2004). Radiation dosimetry of 99mTc-labeled C225 in patients with squamous cell carcinoma of the head and neck. J Nucl Med.
16 Schechter N.R., Yang D.J., Azhdarinia A., Kohanim S., Wendt R., Oh C.S., Hu M., Yu D.F., Bryant J., Ang K.K., Forster K.M., Kim E.E., Podoloff D.A. (2003). Assessment of epidermal growth factor receptor with 99mTc-ethylenedicysteine-C225 monoclonal antibody. Anticancer Drugs.
17 Lundqvist H., Tolmachev V. (2002). Targeting peptides and positron emission tomography. Biopolymers.
18 Niu G., Li Z., Xie J., Le Q.T., Chen X. (2009). PET of EGFR antibody distribution in head and neck squamous cell carcinoma models. J Nucl Med.
19 Nayak T.K., Garmestani K., Baidoo K.E., Milenic D.E., Brechbiel M.W. (2010). Preparation, biological evaluation, and pharmacokinetics of the human anti-HER1 monoclonal antibody panitumumab labeled with 86Y for quantitative PET of carcinoma. J Nucl Med.